# Cy5.5-Trastuzumab

Chemical name: | Cy5.5-Trastuzumab
Abbreviated name: | Cy5.5-Trast
Synonym: | Cy5.5-Herceptin®
Agent category: | Antibody
Target: | Epidermal growth factor receptor-2 (EGFR-2, HER2, erbB-2/neu)
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1064) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20trastuzumab)]

Epidermal growth factor (EGF) is a 53-amino acid cytokine (6.2 kDa) secreted by ectodermic cells, monocytes, kidneys and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF with at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3) and HER4 (erbB-4) (2). HER1, HER3 and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non-small-cell lung, head and neck, and colon cancer (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets (11-13). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350-700 nm) are used. Near-infrared (NIR) fluorescence (700-1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low fluorescence background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive complement to radionuclide imaging in small animals.

Trastuzumab is a humanized IgG_1_ monoclonal antibody (MAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (14). Cardiotoxicity is the most serious complication of using trastuzumab in humans with breast cancer (15). One potential application of a radiolabeled anti-HER2 MAb is the pretreatment imaging of breast cancer patients to predict the therapeutic efficacy of trastuzumab. ^111^In-Trastuzumab and ^68^Ga-F(ab')_2_-trastuzumab have been developed for imaging of human breast cancer (16-19). Trastuzumab has also been successfully coupled with Cy5.5 NIR dye for optical imaging of HER2 density in tumors in mice (20).

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), HER2 (http://www.ncbi.nlm.nih.gov/books?term=HER2%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956), HER2 (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1064))
- Articles in OMIM (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550), HER2 (http://www.ncbi.nlm.nih.gov/omim/164870))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20trastuzumab%20and%20synthesis)]

Commercially available Cy5.5 monofunctional N-hydroxysuccinimide ester was used to conjugate trastuzumab to form Cy5.5-trastuzumab, which was purified by gel-filtration chromatography (20). The molar ratio of Cy5.5 to trastuzumab was estimated to be 2.0-2.5 by spectrometric analyses.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20trastuzumab%20and%20in%20vitro)]

Hilger et al. (20) performed cell-binding assays with Cy5.5-trastuzumab using a human SK-BR-3 breast cancer cells (overexpressing HER2) and normal squamous cell carcinoma cell line PE/CA-PJ34 (normal HER2 expression). Incubation of 0.66 nmol Cy5.5-trastuzumab for 3 h at 4°C showed that a higher fluorescence intensity (a.u.) was observed in the SK-BR-3 cells (1x10^7^ cells, 2133 ± 143 a.u.) than the PE/CA-PJ34 (1x10^7^ cells, 975 ± 95 a.u.). On the other hand, Cy5.5-IgG bindings in both cell types were low (< 500 a.u.) as well as the background fluorescence with buffer alone (~200 a.u.). These results were also confirmed using fluorescence flow cytometry and laser scanning microscopy. No blocking experiment was performed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20trastuzumab%20and%20rodentia)]

Hilger et al. (20) studied the accumulation of Cy5.5-trastuzumab in mice bearing SK-BR-3 (overexpressing HER2) or PE/CA-PJ34 (normal HER2 expression) tumors using whole-body fluorescence detection system. Cy5.5-Trastuzumab (0.66 nmol/mouse) injected intravenously into SCID mice (n = 6) bearing SK-BR-3 tumors (tumor/background = 2.2 ± 0.1) showed distinctly higher fluorescence signals in the SK-BR-3 tumors as compared with PE/CA-PJ34 tumors (tumor/background = 1.3 ± 0.2) in a different group of mice (n = 6) at 16 h after injection. There was a marked intensity of signal in the liver of mice bearing the tumors. Injection of Cy5.5 labeled control IgG in mice (n = 3) bearing the SK-BR-3 tumors revealed tumor/background ratio of 1.4. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20trastuzumab%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20trastuzumab%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy5.5%20trastuzumab%20and%20human)]

No relevant publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
12 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
13 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
14 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
15 Goldenberg M.M. (1999). Trastuzumab, a recombinant DNA-derived humanized monoclonal antibody, a novel agent for the treatment of metastatic breast cancer. Clin Ther.
16 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
17 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
18 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
19 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
20 Hilger I., Leistner Y., Berndt A., Fritsche C., Haas K.M., Kosmehl H., Kaiser W.A. (2004). Near-infrared fluorescence imaging of HER-2 protein over-expression in tumour cells. Eur Radiol.